# ^111^In-Ibritumomab tiuxetan

Chemical name: | ^111^In-Ibritumomab tiuxetan
Abbreviated name: | ^111^In-2B8 MAb
Synonym: | ^111^In-Zevalin®, ^111^In-anti-CD20 antibody, ^111^In-IDEC-2B8 MAb
Agent Category: | Antibody
Target: | CD20 antigen on B-cell non-Hodgkin’s lymphoma
Target Category: | Antibody-antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=115968), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=29773) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=931) for more information about CD20.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zevalin%20OR%20ibritumomab%20OR%20IDEC-2B8)]

^111^In-Ibritumomab tiuxetan (^111^In-2B8) is an immunoconjugate of a murine anti-CD20 monoclonal antibody (MAb) that is chelated to ^111^In for imaging of lymphoid malignancies (1-3). It was approved in the United States in 2002 as a required imaging component of the ^90^Y-ibritumomab tiuxetan therapeutic regimen for the treatment of patients with relapsed or refractory low-grade, follicular, or transformed B-cell non-Hodgkin’s lymphoma (NHL), including patients with rituximab-refractory follicular NHL (4). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The CD20 antigen (Bp35) is a 35-kDa, cell-surface nonglycosylated, hydrophobic phosphoprotein expressed on normal and malignant B-cells, and it does not shed, modulate, or internalize (5-8). It is a transmembrane protein that acts as a calcium channel and plays an important role in cell cycle progression and differentiation of B cells. CD20 is present on approximately 9% of the peripheral blood mononuclear cell fraction and >90% of B-cells from blood and lymphoid organs. Lymphoma cells from >90% of patients with B-cell NHL express this antigen. CD20 is not expressed on uncommitted hematopoietic precursor stem cells. When antibodies bind to this antigen, they induce apoptosis, antibody-dependent cellular cytotoxicity, and complement-dependent cytotoxicity of lymphoma cells. Despite the presence of CD20 on normal B cells, it appears to be a good tumor target for molecular targeting with antibodies for the management of NHL.

Radiolabeled MAbs have been developed for both diagnosis and therapy of tumors (5, 9, 10). Ibritumomab was developed as an anti-CD20 MAb and was characterized by Reff et al. (11). A chimeric 2B8 MAb was constructed and later developed as an United States Food and Drug Administration-approved drug, rituximab (unlabeled MAb), for NHL therapy. Developed from the same 2B8 mouse hybridoma, ibritumomab is an intact murine IgG_1a_ kappa MAb composed of two murine gamma 1 heavy chains (445 amino acids each) and two kappa light chains (213 amino acids each). With the use of tiuxetan (MX-DTPA) as the linker-chelator, ^111^In can be stably linked to ibritumomab for imaging (4, 11, 12). Alternatively, ^90^Y, a pure beta emitter, can be similarly linked to ibritumomab for therapy. MX-DTPA forms a stable covalent urea-type bond with the antibody and chelates the radionuclide via five carboxyl groups and three amino groups (13). Ibritumomab tiuxetan has an approximate molecular mass of 148 kDa. In the Food and Drug Administration approved protocol for the ^90^Y-ibritumomab tiuxetan therapeutic regimen, 250 mg/m^2^ rituximab is given to the patient before the radioactive dose of 185 MBq (5 mCi)/1.6 mg to minimize uptake of ^111^In-2B8 by normal tissue and blood mononuclear cells. An ^111^In-2B8 MAb scan is performed 48-72 h after administration to detect altered biodistribution of the radiolabeled MAb.

The commercial kit for the preparation of ^111^In-ibritumomab tiuxetan contains 3.2 mg/2 ml ibritumomab tiuxetan in 0.9% sodium chloride solution (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed)]

2B8 MAb was synthesized based on the hybridoma technique developed by Kohler and Milstein (14, 15). BALB/c mice were immunized with the human lymphoblastoid cell line SB (4, 16). Spleens were isolated from mice with high serum titers of anti-CD20 antibodies, and the splenocytes were fused with the mouse myeloma SP2/0. Brechbiel and Gansow (12) synthesized the MX-DTPA [2-(p-isothiocyanatobenzyl)-6-methyldiethylenetriaminepentaacetic acid] chelator by substituting a 4-isothiocyanatobenzyl group onto the carbon backbone of DTPA. Methyl groups were strategically incorporated onto the backbone of the ligand via a peptide synthesis route. In the commercial preparation, 203.5 MBq (5.5 mCi) of ^111^In chloride buffered by 50 mM sodium acetate (1.5 times the volume of ^111^In chloride) is reacted with 1.6 mg/ml 2B8 MAb for 30 min. A formulation buffer containing human albumin is used to terminate the reaction and to protect the radiolabeled product from radiolysis (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Zevalin%20or%20ibritumomab%20or%20IDEC-2B8%29%20AND%20in%20vitro)]

Chinn et al. (16) used flow cytometry to show that 2B8 MAb was specific for B cells and did not react with other T cells, monocytes, and macrophages. ^111^In-2B8 MAb was prepared with a specific activity (sa) of 111 MBq/mg (3 mCi/mg) and it exhibited no apparent loss of immunoreactivity compared with the unlabeled 2B8 MAb. An in vitro stability study indicated that the immunoreactivity was retained for incubation times up to 48 h at 4^o^C. The apparent affinity (K_d_) of ibritumomab tiuxetan for CD20 was 14-18 nM (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Zevalin%20or%20IDEC-2B8%20or%20ibritumomab%29%20AND%20rodentia)]

The biodistribution of 37 kBq (1 µCi) of ^111^In-2B8 MAb with a specific activity of 111 MBq/mg (3 mCi/mg) in mice was determined by Chinn et al. (16). The highest level of radioactivity was in the blood and decreased from 40.3 ± 5.3% injected dose (ID)/g (n = 5) at 1 h to 19% ID/g at 72 h. The lungs and liver had the next highest levels with 14.2 ± 1.4% ID/g and 10.3 ± 1.6% ID/g at 1 h, respectively, which decreased to 7.6 ± 0.3% ID/g and 9.9 ± 1.8% ID/g at 72 h, respectively. The localization of 617.9 kBq (16.7 µCi) of ^111^In-2B8 MAb in athymic mice (n = 3) bearing Ramos B cell tumors showed that the radioactivity in the tumor steadily increased from 0.5 ± 0.2% ID/g at 1 h to 13.4 ± 1.0% ID/g at 72 h, and the tumor/muscle ratio increased from 1.5 ± 0.6 at 1 h to 20.6 ± 7.2 at 72 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ibritumomab%20or%20Zevalin%20or%20IDEC-2B8%29%20AND%20human)]

In a Phase III trial of ^90^Y-2B8 MAb therapy, patients with histologically confirmed, relapsed or refractory low-grade, follicular, or transformed CD20+ B-cell NHL received an infusion of 250 mg/m^2^ rituximab and then an imaging dose of 185 MBq (5 mCi) of ^111^In-2B8 MAb (13). The median biological blood t_½_ of the antibody was 47 h and the median blood residence time was 26 h. The fraction of injected radioactivity excreted in urine over 7 days was estimated to be 8.3%. In another study, ^111^In-2B8 MAb detected 56% and 92% of known tumor sites when the patients were pretreated with unlabeled 2B8 MAb doses of 1.0 and 2.5 mg/kg, respectively (4). In comparison, only 18% of known sites of disease were detected when no unlabeled 2B8 MAb was administered.

The dosimetry of ^111^In-2B8 MAb has been estimated with use of sequential whole body images and the MIRDOSE 3 software program (13, 17). The distribution of ^111^In-2B8 MAb showed moderately high radioactivity in the liver and spleen, and relatively low radioactivity in the kidneys, urinary bladder and bowel. The spleen received the highest absorbed radiation dose, 0.9 mGy/MBq (3333 mrad/mCi), and the bone marrow received 0.2 mGy/MBq (741 mrad/mCi). The liver received the second highest dose, 0.7 mGy/MBq (2590 mrad/mCi), and both the lower large intestinal wall and the heart wall received 0.4 mGy/MBq (1481 mrad/mCi). The urinary bladder wall and the kidneys received only 0.2 mGy/MBq (741 mrad/mCi).

Conti et al. (18) reported the results of the ^111^In-2B8 MAb imaging registry as a component of the ^90^Y-2B8 MAb therapy for 953 patients who were treated between March 2002 and March 2003. Altered biodistribution was reported in <0.6% of cases and involved mostly prominent bone marrow uptake. In these cases, imaging appeared to help prevent the delivery of excessive radiation to the bone marrow.

Various other studies have been published on the dosimetry and efficacy of the therapeutic application of treating NHL with ^90^Y-2B8 MAb [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Zevalin%20or%20ibritumomab%20or%20IDEC-2B8%29%20AND%20human%20and%20therapy%29)].

## References

1 (2002). Ibritumomab tiuxetan (Zevalin) for non-Hodgkin's lymphoma. Med Lett Drugs Ther.
2 (2002). Targeted treatment for non-Hodgkin's lymphoma. Health News.
3 (2002). First radiopharmaceutical for non-Hodgkin's lymphoma. FDA Consum.
4 Zevalin. Ibritumomab tiuxetan. Prescribing Information. biogen idec, 2005. 3-1074-247: p. 1-11.
5 Hainsworth JD. (2000). Monoclonal antibody therapy in lymphoid malignancies. Oncologist.
6 Tobinai K. (2002). Rituximab and other emerging monoclonal antibody therapies for lymphoma. Expert Opin Emerg Drugs.
7 Tobinai K. (2003). Rituximab and other emerging antibodies as molecular target-based therapy of lymphoma. Int J Clin Oncol.
8 Zelenetz AD A clinical and scientific overview of tositumomab and iodine I 131 tositumomab Semin Oncol 2003 30 2 Suppl 4 22 30 12728404
9 Kowalsky RJ, Falen SW. (2004).
10 Wu AM, Senter PD. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
11 Reff ME, Carner K, Chambers KS, Chinn PC, Leonard JE, Raab R, Newman RA, Hanna N, Anderson DR. (1994). Depletion of B cells in vivo by a chimeric mouse human monoclonal antibody to CD20. Blood.
12 Brechbiel MW, Gansow OA. (1991). Backbone-substituted DTPA ligands for 90Y radioimmunotherapy. Bioconjugate Chem.
13 Wiseman GA, White CA, Sparks RB, Erwin WD, Podoloff DA, Lamonica D, Bartlett NL, Parker JA, Dunn WL, Spies SM, Belanger R, Witzig TE, Leigh BR. (2001). Biodistribution and dosimetry results from a phase III prospectively randomized controlled trial of Zevalin radioimmunotherapy for low-grade, follicular, or transformed B-cell non-Hodgkin's lymphoma. Crit Rev Oncol Hematol.
14 Kohler G, Milstein C. (1975). Continuous cultures of fused cells secreting antibody of predefined specificity. Nature.
15 Stashenko P, Nadler LM, Hardy R, Schlossman SF. (1980). Characterization of a human B lymphocyte-specific antigen. J Immunol.
16 Chinn PC, Leonard JE, Rosenberg J, Hanna N, Anderson DR. (1999). Preclinical evaluation of 90Y-labeled anti-CD20 monoclonal antibody for treatment of non-Hodgkin's lymphoma. Int J Oncol.
17 Wiseman GA, White CA, Stabin M, Dunn WL, Erwin W, Dahlbom M, Raubitschek A, Karvelis K, Schultheiss T, Witzig TE, Belanger R, Spies S, Silverman DH, Berlfein JR, Ding E, Grillo-Lopez AJ. (2000). Phase I/II 90Y-Zevalin (yttrium-90 ibritumomab tiuxetan, IDEC-Y2B8) radioimmunotherapy dosimetry results in relapsed or refractory non-Hodgkin's lymphoma. Eur J Nucl Med.
18 Conti PS Radioimmunotherapy with yttrium 90 ibritumomab tiuxetan (Zevalin): the role of the nuclear medicine physician Semin Nucl Med 2004 34 1 Suppl 1 2 3 14762737